# Trastuzumab-rhodamine green

Chemical name: | Trastuzumab-rhodamine green
Abbreviated name: | Trast-RhodG
Synonym: | Herceptin-RhodG
Agent Category: | Antibody
Target: | EGF HER2 receptor
Target Category: | Antibody binding to EGF receptor
Method of detection: | Optical fluorescence imaging
Source of signal/contrast: | Rhodamine green (RhodG)
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RhodG%20and%20HER2)]

Epidermal growth factor (EGF) is a cytokine (6.2 kDa) composed of 53 amino acids that is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant of 0.1 nM (11). Trastuzumab is approved for clinical use in anti-cancer therapies in both Europe and North America [FDA package insert (http://www.fda.gov/cder/foi/label/2000/trasgen020900LB.htm)]. One potential application of a radiolabeled anti-HER2 mAb is pretreatment imaging of breast cancer patients to predict the therapeutic efficacy of trastuzumab. ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging human breast cancer (12-16). Optical fluorescence imaging is increasingly used to study biological functions of specific targets (17, 18) and is becoming a non-invasive alternative to radionuclide imaging in small animals. Trastuzumab-rhodamine green (Trast-RhodG) has been prepared to study the vasculature of the tumor in tumor-bearing mice (19). Rhodamine green is an optical fluorescence dye with an absorbance maximum at 502 nm, an emission maximum at 527 nm, and an extinction coefficient of 75,000 M^-1^cm^-1^. Trast-RhodG has been found to have a high tumor accumulation in an animal model of lung metastases in mice.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RhodG%20and%20HER2%20and%20engineered)]

Koyama et al. (19) prepared trast-RhodG by incubating trastuzumab with Rhoda-succinimidyl ester in DMSO for 15 min. Trast-RhodG was isolated with column chromatography. There is ~1 RhodG molecule per trastuzumab molecule.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RhodG%20and%20HER2%20and%20in%20vitro)]

Koyama et al. (19) performed cell-binding assays with trast-RhodG using gene-transfected murine embryonic fibroblast 3T3/HER2^+^ cells with HER2 overexpression. Fluorescence flow cytometry after 1 h of incubation showed a mean fluorescence intensity value of 453 absorbance units, which increased gradually up to 8 h. Trast-RhodG retained the high mean fluorescence intensity values at 8 h of incubation in tracer-free medium. Fluorescence microscopy analysis indicated that trast-RhodG was internalized into the cells. A control antibody (HUT-RhodG) did not bind to the 3T3/HER2+ cells, whereas trast-RhodG did not bind to 3T3/HER2^-^ cells. No blocking experiment was performed.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RhodG%20and%20HER2%20and%20rodentia)]

Koyama et al. (19) studied the accumulation of trast-RhodG in mice bearing 3T3/HER2^+^ or 3T3/HER2^-^lung metastases using a spectral fluorescence imaging system after i.v. injection of ~0.4 nmol trast-RhodG. Accumulation of trast-RhodG in 3T3/HER2^+^ tumor foci was observed at 1, 2, 4, and 7 days after injection, whereas no accumulation was detected in 3T3/HER2^-^ tumor foci. No accumulation of the HUT-RhodG control antibody was observed in the 3T3/HER2^+^ tumor foci. The spectral fluorescence imaging had a sensitivity of 100% (490 of 490 foci) and a specificity of 96% (705 of 732 foci). No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RhodG%20and%20HER2%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RhodG%20and%20HER2%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RhodG%20and%20HER2%20and%20human)]

No publication is currently available.

## NIH Support

Intramural Research Program

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
18 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
19 Koyama Y., Hama Y., Urano Y., Nguyen D.M., Choyke P.L., Kobayashi H. (2007). Spectral fluorescence molecular imaging of lung metastases targeting HER2/neu. Clin Cancer Res.